# [^18^F]Fluorobenzoyl-((VHPKQHRGGSY)_2_K)_2_KK

Chemical name: | [^18^F]Fluorobenzoyl-((VHPKQHRGGSY)_2_K)_2_KK
Abbreviated name: | [^18^F]4V
Synonym:
Agent category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-4V)]

Endothelial cells are important cells in inflammatory responses (1-2). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase secretion of tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

VCAM-1 is found in very low amounts on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (4-8). VCAM-1 binds to the very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (9). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression to vulnerable plaques, which may erode and rupture. Cross-linked iron oxide nanoparticles targeted with anti-VCAM-1 antibody are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (10). A tetrameric linear peptide, ((VHPKQHRGGSY)_2_K)_2_KK (TLP), was identified with phage screening against VCAM-1 and radiolabeled with 4-[^18^F]fluorobenzaldehyde ([^18^F]FBA) to form [^18^F]fluorobenzoyl-TLP ([^18^F]4V) as a potential positron emission tomography (PET) imaging agent to target atherosclerotic plaques and myocardial ischemic lesions (11).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=VCAM-1)
- Clinical trials (VCAM-1 (http://www.clinicaltrials.gov/ct2/results?term=VCAM-1))
- Drug information in FDA (http://google2.fda.gov/search?q=VCAM-1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=11)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+synthesis)]

Nahrendorf et al. (11) reported the synthesis of [^18^F]4V. The tetrameric linear peptide, TLP, was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. TLP was then reacted with [^18^F]FBA to form [^18^F]4V using an automated synthesizer. [^18^F]4V was purified with high-performance liquid chromatography. The specific activity, radiochemical purity, radiolabeling yield, and total time of synthesis of [^18^F]4V were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+in+vitro)]

Nahrendorf et al. (11) measured the binding affinity of TLP to human VCAM-1 with a 50% inhibition concentration (IC_50_) value of 87 nM (349-fold better than the linear monomer) using ^99m^Tc-DOTA-TLP as a ligand tracer. The accumulation of [^18^F]4V (100 ng) in murine heart endothelial cells in culture was inhibited by >95% with 1 µg murine soluble VCAM-1. Incubation of [^18^F]4V with excised aortas from wild-type mice, apoE^-/-^ mice, and apoE^-/-^ mice treated with atorvastatin showed that aortas from apoE^-/-^ mice exhibited >2-fold higher radioactivity than the aortas from wild-type mice and apoE^-/-^ mice treated with atorvastatin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+rodentia)]

Nahrendorf et al. (11) performed ex vivo biodistribution studies in wild-type mice (n = 6) at 4 hr after injection. Each mouse received 5.55 MBq (0.15 mCi) [^18^F]4V. The organ/tissue with the highest accumulation (percent injected dose per gram (% ID/g)) was the kidney (13.2 ± 2.8), followed by the liver (3.7 ± 1.1), lymph node (3.7 ± 0.3), lung (2.2 ± 0.8), spleen (2.1 ± 0.6), small intestine (1.9 ± 0.4), skin (1.7 ± 0.6), stomach (1.7 ± 1.1), blood (1.5 ± 0.4), large intestine (1.4 ± 0.5), aorta (1.3 ± 0.4), bone (1.3 ± 0.4), skeletal muscle (0.7 ± 0.3), heart (0.6 ± 0.2), and feces (0.2 ± 0.1). Dynamic PET/CT imaging of apoE^-/-^ mice (n = 8) was conducted with intravenous injection of 13 MBq (0.35 mCi) [^18^F]4V for 7 h. Strong focal signal in the aortic root was identified at 1–2 h with an aorta/blood ratio of 2. Atorvastatin treatment blocked the signal increase to near the signal expression of the wild-type aortas (P < 0.05). [^18^F]4V radioactivity correlated with VCAM-1 mRNA levels (R = 0.79, P = 0.03) in the excised aortas.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-4V+human)]

No publication is currently available.

## NIH Support

R01 HL078641, R24 CA092782, U01 HL080731

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
5 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
6 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
7 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
8 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
9 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
10 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.
11 Nahrendorf M., Keliher E., Panizzi P., Zhang H., Hembrador S., Figueiredo J.L., Aikawa E., Kelly K., Libby P., Weissleder R. (2009). 18F-4V for PET-CT imaging of VCAM-1 expression in atherosclerosis. JACC Cardiovasc Imaging.